# Cbz-Phe-Lys(Cy5)-methyl ketone-2,6,dimethylterephthalic amide-hexyl-QSY 21

Chemical name: | Cbz-Phe-Lys(Cy5)-methyl ketone-2,6,dimethylterephthalic amide-hexyl-QSY 21
Abbreviated name: | GB137
Synonym:
Agent category: | Small molecule
Target: | Cysteine cathepsin
Target category: | Enzyme
Method of detection: | Optical imaging
Source of signal/contrast: | Cy5
Activation: | Yes
Studies: | - In vitro; - Rodents | No structure is currently available in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=GB137)]

Cysteine cathepsins are proteolytic enzymes that belong to the papain subfamily of cysteine proteases (1). The human family of cysteine cathepsins consists of 11 members: cysteine cathpsin B, C, F, H, K, L, O, S, V, W and X (2). The active site in these enzymes contains a cysteine residue that acts as a nucleophile for attacking the peptide bond of substrates, and a His residue that acts as a general base for shuttling protons (3). As a key component in cell division, cell death and antigen presentation, cysteine cathepsins are found to be associated with various diseases, including cancer, arthritis, osteoporosis, cardiovascular diseases and neurodegenerative disorders (4). Increased expression, activity and mislocation of several cysteine cathepsins (B and L) are significantly correlated with malignant progressions in tumors (2). Like the other four catalytic types of mammalian protease (aspartic, metallo, serine and threonine), the cysteine cathepsins are synthesized as inactive zymogens and their activity is post-translationally regulated (5). Thus, the abundance of these enzymes may not directly correlate to their proteolytic activity. Activity-based proteomics is a novel technology that has been developed recently to characterize the activity of proteolytic enzymes (6, 7). In this method, small molecules known as activity-based probes (ABPs) covalently bind to the catalytic site of specific target enzymes in complex proteomes. ABPs comprise three basic elements: a reactive functional group known as a warhead for labeling enzymes via covalent binding, a linker for preventing steric congestions, and a reporter tag for identification, purification and visualization of the probe-labeled enzymes (8). For instance, acyloxymethyl ketone (AOMK) is a warhead specific for cysteine cathepsins (B, L and S). The ketone in AOMKs reacts with the cysteine in the enzyme active via a sulfhydryl nucleophile to produce a stable thiomethyl ketone adduct, leading to blockade of cysteine cathepsins (8). With an optical labeling as the tag, the ABPs can be used to image the activity of proteolytic enzymes in vivo (1).

CBz-Phe-Lys(Cy5)-methyl ketone-2,6,dimethylterephthalic amide-hexyl-QSY 21(GB137) is an optical agent used for imaging cysteine cathepsins in vivo (1). GB137 consists of four components: an AOMK type of warhead to bind specifically to cysteine cathepsin B and cysteine cathepsin L, a hexyl and a Lys as spacers to reduce steric congestion, the infrared fluorescent probe Cy5 (646/664 nm excitation/emission), and the commercial fluorescence quencher QSY 21 (absorption ~661 nm). As a quenched ABP (qABP), Cy5 and QSY 21 are separated by a Lys-methyl ketone in the molecule. In the absence of cysteine cathepsin, the fluorescence emitted by the Cy5 is quenched by the QSY 21, and no fluorescence is observed. Upon binding to the enzyme, GB137 interacts with the enzyme active site to release the quenching group QSY 21 as a side product, and produces a Cy5-labeled cysteine cathepsin that is detectable with infrared fluorescent imaging.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=( GB137)+AND+synthesis%0D%0A)]

Blum et al. reported the details of the synthesis of GB137 in multiple steps (1). Initially, 2-chloritrityl chloride resin was loaded with the commercial Fmoc 1, 6-diaminohexane hydrochloride in the presence of diisopropylethylamine (DIEA) in anhydrous dichloromethane (DCM). Then, the Fmoc was removed with 20% piperidine/dimethylformamide (DMF) (v/v). The produced resin-attached 6-aminohexane was reacted with 2, 6-dimethylterephthalic acid in the presence of DIEA, hydroxybenzotriazole (HOBT) and benzotriazol-1-yl-oxytripyrrolidinophosphonium hexafluorophosphate (PyBOP) to yield resin-attached 2,6-dimethyl-4-(6-aminohexocarbonyl) benzoic acid. The carboxyl terminus was further conjugated with N-a-Fmoc-Lys (N-ε-Boc)-chloromethyl ketone in DMF to produce a resin-attached AOMK. After removal of the N-α-Fmoc with 5% diethanolamine(DEA)/DMF(v/v), CBz-protected Phe (ZF) was coupled to the N-α-amine in the Lys using solid-phase peptide synthesis in the presence of HOBT and disopropylcarbodiimide (DIC). The resulting ZF-Lys(N-ε-Boc)-2,6 dimethylterephthalic amide 6-aminohexane was released from the resin with 1% trifluoroacetic acid /DCM. In the presence of N, N-diisopropylethylamine (DIPEA), the released product (1.1% yield) was sequentially coupled with QSY 21 succinimidyl ester at the 6-aminohexane (75% yield) and with Cy5 succinimidyl ester at the N-ε-free amine of Lys (65% yield) to produce GB137 as a blue powder. The molecular weight of GB137 was determined to be 2019.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=( GB137)+AND+%22in+vitro%22)]

Blum et al. examined the specificity of GB137 for in vitro labeling of cysteine cathepsins (1). A series of cancer cells was used, including oncogene Hras1 transfected mouse skeletal myoblast cells (C2C12/Hras1), human breast cancer cells (MDA-MD 231, MDA-MB 435 and MDA-MB 231 MFP), murine fibroblast cells (NIH-3T3), and human glioblastoma cells (U87MG). These cells were pretreated with 5 μM GB111-NH_2_, a potent cysteine cathepsin inhibitor, for 1.5 h, followed by incubation with 1.5 μM GB137 for 3 h. Then, the cells were lysed with a dounce homogenizer in detergent buffer. The obtained crude lysates were separated with SDS-PAGE, and visualized with fluorescent scanning to examine the GB137-labeled cysteine cathepsins. In all these cell lines, specifically labeled cysteine cathepsins were observed to be 20-30 kDa in size, which corresponded to GB137-labeled cysteine cathepsins B and/or L. However, the amount of labeled cysteine cathepsins varied over more than 10-fold, with the highest appeared in the C2C12/Hras1 cells. MDA-MD 231 cells, MDA-MB 435 cells, and MDA-MB 231 MFP cells exhibited a similar pattern for cysteine cathepsins with moderate amplitudes. As a control, GB137 was incubated with serum for 4 h to test its sensitivity to serum. No change in the labeling activity of GB137 was observed.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=( GB137) +AND++rodentia)]

Blum et al. examined the pharmacokinetics of GB137 in vivo with fluorescent imaging (1). BALB/c nude mice (n=3) were subcutaneously implanted with MDA-MB 231 MFP cells at ventral and dorsal locations. Two weeks later, the mice were injected intravenously with 2 μg/g GB137. After injection, fluorescent images were collected with a charge-coupled device (CCD) camera at various time points over a 24 h period. GB137 generated a specific signal in the tumor location that increased with time and reached a maximum by 6-8 h after the injection. After collecting the images from the last imaging time point, the mice were euthanized and tissues were harvested for protein extraction. The extracts were separated with SDS-PAGE and visualized with fluorescent scanning. GB137-labeled cysteine cathepsins B and L were found in the tissues of tumors, liver, spleen and kidney.

Blum et al. used GB137 to evaluate the in vivo efficacy of small-molecule inhibitors for cysteine cathepsins with fluorescent imaging (1). BALB/c nude mice (n=3)with MDA-MB 231 MFP were treated with the general inhibitor of protease N-methyl-piperazine-phenylalanyl-homophenylalanyl-vinylsulfone phenyl (K11777) at a dose of 50 mg/kg twice daily starting at 5 d before the imaging in order to reduce cathepsin activity in tumor tissues. As a control, two mice bearing tumors were treated with DMSO vehicle. Mice were intravenously injected with 25 nmol GB137, and images were obtained at various times up to 10 h. At 10 h, the signal was reduced by 60-80% in the mice treated with K11777 compared to the control mice. To further confirm this observation, the mice were euthanized and the tissues were harvested for analysis. The tumor tissues were imaged with the same CCD camera. The signal intensity in the tumors treated with K11777 exhibited a reduced signal. All tissues were then lysed for protein extraction. The extracts were separated with SDS-PAGE. The GB137 labeled cysteine cathepsins were quantified, which demonstrated that the labeling of specific cysteine cathepsins was inhibited by 50-80% in tissues from the mice treated with K11777 compared to the control mice.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22%20SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=( GB137) +AND+(primate+non+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=( GB137) +AND+human)]

No publication is currently available.

### NIH Support

RR 20843, EB 05011, CA 72006

## References

1 Blum G., von Degenfeld G., Merchant M.J., Blau H.M., Bogyo M. (2007). Noninvasive optical imaging of cysteine protease activity using fluorescently quenched activity-based probes. Nat Chem Biol.
2 Palermo C., Joyce J.A. (2008). Cysteine cathepsin proteases as pharmacological targets in cancer. Trends Pharmacol Sci.
3 Stoka V., Turk B., Turk V. (2005). Lysosomal cysteine proteases: structural features and their role in apoptosis. IUBMB Life.
4 Blum G., Mullins S.R., Keren K., Fonovic M., Jedeszko C., Rice M.J., Sloane B.F., Bogyo M. (2005). Dynamic imaging of protease activity with fluorescently quenched activity-based probes. Nat Chem Biol.
5 Blum G. (2008). Use of fluorescent imaging to investigate pathological protease activity. Curr Opin Drug Discov Devel.
6 Saghatelian A., Cravatt B.F. (2005). Assignment of protein function in the postgenomic era. Nat Chem Biol.
7 Evans M.J., Cravatt B.F. (2006). Mechanism-based profiling of enzyme families. Chem Rev.
8 Paulick M.G., Bogyo M. (2008). Application of activity-based probes to the study of enzymes involved in cancer progression. Curr Opin Genet Dev.